# ^99m^Tc-Hydrazinonicotinyl(tricine)(TPPTS)-Glu-c(RGDyK)-bombesin[7-14]NH_2_

Chemical name: | ^99m^Tc- Hydrazinonicotinyl(tricine)(TPPTS)-Glu-c(RGDyK)-bombesin[7-14]NH_2_
Abbreviated name: | ^99m^Tc-HYNIC-RGD-BBN
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR), integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal\contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-Rs) have been identified on CNS and GI tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (7). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (8-13). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various ligands have been introduced for imaging of tumors and tumor angiogenesis (14).

Because breast and prostate cancers express both GRPR and α_v_β_3_, Liu et al. (15) designed an RGD-BBN heterodimer in which BBN[7-14]NH_2_ and c(RGDyK) are connected with a glutamate linker (BBN on the Glu side chain γ-carboxylate group and RGD on the Glu side chain α-carboxylate group). 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA) was used as a bifunctional chelator for labeling RGD-BBN to form ^64^Cu-NOTA-RGD-BBN (http://www.ncbi.nlm.nih.gov/books/NBK23431/) for use in positron emission tomography (PET) imaging of α_v_β_3_ and GRPR in nude mice bearing human tumors. For single-photon emission computed tomography (SPECT), Liu et al. (16) conjugated Glu-RGD-BBN with 6-hydrazinonicotinyl (HYNIC) and labeled the product with ^99m^Tc, using tricine and trisodium triphenylphosphine-trisulfonate (TPPTS) as the coligands. ^99m^Tc-HYNIC-RGD-BBN was evaluated in C57/BL6 mice bearing mouse Lewis lung carcinomas (LLC).

### Related Resource Links:

- Chapters in MICAD (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=(GRPR%20OR%20GRP-R)%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/gene/2925), GRP (http://www.ncbi.nlm.nih.gov/gene/2922), α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GRPR (http://www.ncbi.nlm.nih.gov/omim/305670), GRP (http://omim.org/entry/137260), α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (GRPR (http://www.clinicaltrials.gov/ct2/results?term=bombesin), RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+synthesis)]

RGD-BBN was prepared with solid-phase peptide synthesis (16). Addition of a HYNIC group to RGD-BBN was performed by mixing 2 µmol RGD-BBN with 6 µmol HYNIC-NHS in sodium bicarbonate buffer (pH 9) for 5 h at room temperature. HYNIC-RGD-BBN was isolated with high-performance liquid chromatography (HPLC), with 56% yield. Measurement with matrix-assisted laser desorption ionization/time of flight mass spectrometry indicated the molecular mass to be m/z 1,918.60 (calculated molecular weight, 1,919.17). For ^99m^Tc labeling, a solution of 370 MBq (10 mCi) Na^99m^TcO_4_, SnCl_2_, and 10 nmol HYNIC-RGD-BBN in succinate buffer (pH 5) was incubated for 10 min at 25°C. After addition of TPPTS, the mixture was heated for 30 min at 100°C. ^99m^Tc-HYNIC-RGD-BBN was isolated with HPLC, with 90% yield and a radiochemical purity of >98%. The specific activity was >30 MBq/nmol (0.81 mCi/nmol). The total preparation time was ~50 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+in+vitro)]

Liu et al. (16) performed in vitro inhibition studies of HYNIC-RGD-BBN in cultured U87MG cells with ^125^I-c(RGDyK). The 50% inhibition concentration (IC_50_) values were 18.8 ± 3.8 nM and 10.8 ± 2.6 nM for HYNIC-RGD-BBN and c(RGDyK), respectively. In vitro inhibition studies of HYNIC-RGD-BBN were also performed in cultured PC-3 cells (high GRPR and moderate α_v_β_3_ levels) with ^125^I-[Tyr^4^]-BBN; the IC_50_ values were 104.7 ± 5.8 nM and 71.6 ± 3.1 nM for HYNIC-RGD-BBN and BBN, respectively. The HYNIC-RGD-BBN heterodimer exhibited slightly lower binding affinities for the GRPR and α_v_β_3_ integrin receptor than the corresponding unconjugated RGD and BBN peptides. Cellular accumulation of ^99m^Tc-HYNIC-RGD-BBN in PC-3 tumor cells showed a gradual increase in radioactivity in PC-3 cells from 30 min to 4 h. The cellular radioactivity reached 4.0% of incubation dose at 4 h. Treatment with excess RGD-BBN (1,000 nM) almost completely inhibited the accumulation of ^99m^Tc-HYNIC-RGD-BBN in PC-3 tumor cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+%20rodentia)]

Gamma planar imaging scans were performed in mice (n = 4/group) bearing LLC at 1 h after intravenous injection of 14.8 MBq (400 μCi) ^99m^Tc-HYNIC-RGD-BBN (16). The tumors and kidneys were clearly visualized. Blocking studies were performed with coinjection of BBN (15 mg/kg), cRGDyK (10 mg/kg), or BBN (15 mg/kg) plus cRGDyK (10 mg/kg). Tumor accumulation of ^99m^Tc-HYNIC-RGD-BBN exhibited little change with BBN, whereas cRGDyK or BBN plus cRGDyK completely blocked the radioactivity in the tumors. Gamma planar imaging scans were performed in mice (n = 4/group) bearing LLC and inflammation at 1 h after injection of ^99m^Tc-HYNIC-RGD-BBN or [^18^F]Fluoro-2-deoxy-2-D-glucose ([^18^F]FDG (http://www.ncbi.nlm.nih.gov/books/NBK23335/)) High radioactivity levels were observed with FDG in both inflammation sites and LLC tumors, whereas only LLC tumors were visualized with ^99m^Tc-HYNIC-RGD-BBN. Whole-body SPECT/CT imaging studies were also performed in mice (n = 4) bearing LLC at 1.5 h and 3 h after intravenous injection of 37 MBq (1 mCi) ^99m^Tc-HYNIC-RGD-BBN. Predominant kidney, tumor, and pancreas accumulation of ^99m^Tc-HYNIC-RGD-BBN was clearly visualized. The pulmonary metastatic lesions were clearly visualized and verified by anatomical examination and histostaining.

Liu et al. (16) performed ex vivo biodistribution studies in mice (n = 4/group) bearing LLC at 1 h and 2 h after injection of 0.37 MBq (0.01 mCi) ^99m^Tc-HYNIC-RGD-BBN. Tumor accumulation of ^99m^Tc-HYNIC-RGD-BBN was 2.69 ± 0.66% injected dose/gram (ID/g) at 1 h and 1.99 ± 0.61% ID/g at 2 h after injection. The inflammation accumulation of ^99m^Tc-HYNIC-RGD-BBN was 1.20 ± 0.32% ID/g at 1 h after injection and 0.56 ± 0.17% ID/g at 2 h after injection. The organ with the highest accumulation at 1 h after injection was the pancreas (26% ID/g), followed by the kidney (17% ID/g), intestine (10% ID/g), and stomach (5% ID/g). The liver, heart, bone, blood, and muscle exhibited <1% ID/g. Co-injection with excess RGD-BBN blocked radioactivity in the pancreas, intestine, stomach, and tumor, whereas little inhibition was observed in the inflammation. [^18^F]FDG showed high heart (23.5% ID/g) and kidney (36.0% ID/g) accumulation of radioactivity. The tumor and inflammation accumulation of [^18^]FDG was 6.56 ± 2.27% ID/g and 5.94 ± 2.35% ID/g, respectively. The tumor/inflammation and tumor/muscle ratios of [^18^F]FDG were >one-fold lower than those of ^99m^Tc-HYNIC-RGD-BBN (P < 0.05).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+human)]

No publication is currently available.

## NIH Support

R01 CA120188, R01 CA119053, R21 CA121842, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
7 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
8 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
9 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
10 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
11 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
12 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
13 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
14 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
15 Liu Z., Yan Y., Chin F.T., Wang F., Chen X. (2009). Dual integrin and gastrin-releasing peptide receptor targeted tumor imaging using 18F-labeled PEGylated RGD-bombesin heterodimer 18F-FB-PEG3-Glu-RGD-BBN. J Med Chem.
16 Liu Z., Huang J., Dong C., Cui L., Jin X., Jia B., Zhu Z., Li F., Wang F. (2012). 99mTc-labeled RGD-BBN peptide for small-animal SPECT/CT of lung carcinoma. Mol Pharm.